# L-3,4-Dihydroxy-6-[^18^F]fluorophenylalanine

Chemical name: | L-3,4-Dihydroxy-6-[^18^F]fluorophenylalanine
Abbreviated name: | 6-[^18^F]Fluoro-L-DOPA, [^18^F]FDOPA, FDOPA
Synonym:
Agent category: | Amino acid
Target: | Aromatic L-amino acid decarboxylase; L-type amino acid transporter system
Target category: | Enzyme; transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDOPA%5BAll%20Fields%5D)]

Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in striatum of the brain (1, 2). PD is caused by a shortage of dopamine. Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition and emotion. Dopamine also plays a role in various neuropsychiatric disorders, such as schizophrenia, autism, attention deficit hyperactivity disorder, and drug abuse.

Dopamine is synthesized within nerve cells (3). L-tyrosine is converted to dihydroxyphenylalanine (L-DOPA) and then to dopamine in a two-step process. The first, rate limiting step is catalyzed by tyrosine 3-monoxygenase (tyrosine hydroxylase or TH). The second step is catalyzed by aromatic L-amino acid decarboxylase (L-DOPA decarboxylase, AAAD). In parts of the nervous system that release dopamine as a neurotransmitter (dopaminergic neurons), no further metabolism occurs and dopamine is stored in vesicles in the presynaptic nerve terminals by virtue of the dopamine reuptake transporter, DAT.

6-[^18^F]Fluoro-L-DOPA (FDOPA) is a radiolabeled analog of L-DOPA used to evaluate the central dopaminergic function of pre-synaptic neurons using positron emission tomography (PET) (4, 5). FDOPA PET reflects DOPA transport into the neurons, DOPA decarboxylation and dopamine storage capacity. The tracer is converted to 6-[^18^F]fluorodopamine (FDA) by AAAD and retained in the striatum. FDA can be O-methylated by catechol-O-methyltransferase (COMT) to 3-O-methyl-6-[^18^F]fluoro-L-dopa (3-OMFD), which is uniformly distributed throughout the brain. FDA is also metabolized via monoamine oxidase to yield [^18^F]6-fluoro-3,4-dihydroxyphenylacetic acid (FDOPAC) and subsequently by COMT to yield [^18^F]6-fluorochomovanillic acid (FHVA). AAAD and COMT are also present in peripheral tissues such as liver, kidneys, and lung. In clinical studies, AAAD is commonly inhibited with carbidopa, whereas COMT is blocked by entacapone and nitecapone. These two types of inhibitors enhance the availability of FDOPA in the brain.

### Related Resource Links:

- Chapters in MICAD (Amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D), dopamine (http://www.ncbi.nlm.nih.gov/books/?term=Dopamine+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books))
- Gene information in NCBI (L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428), aromatic L-amino acid decarboxylase (http://www.ncbi.nlm.nih.gov/gene/1644))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D), aromatic L-amino acid decarboxylase (http://omim.org/entry/107930))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters), FDOPA (http://www.clinicaltrials.gov/ct2/results?term=FDOPA))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15), FDOPA (http://google2.fda.gov/search?q=FDOPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDOPA%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

FDOPA can be synthesized by either electrophilic or nucleophilic process (6). Regioselective electrophilic fluorodemetallation of either a mercuryl or a trimethylstannyl precursor is rapid and simple. Electrophilic fluorination of L-methyl-N-acetyl-[methoxy-4-acetoxyphenyl]alanine with [^18^F]acetyl hypofluorite to provide FDOPA in 8% radiochemical yield at the end of bombardment after hydrolysis and high-performance liquid chromatography (HPLC) purification (7). An overall synthesis time is 100 min with a 95% chemical purity and a specific activity of 7.4 GBq/mmol (200 mCi/mmol) at the end of synthesis (EOS). A robotic synthesis was performed using [^18^F]F_2_/neon gas and the trimethylstannyl precursor in about 110 min (8). The radiochemical purity was >97% and the specific activity was 2.59 GBq/mmol (70 mCi/mmol) at the EOS. The radiochemical yield was about 8.2% (uncorrected for decay)

A multi-step synthesis, based on the nucleophilic displacement of a nitro group using the standard [^18^F] potassium Kryptofix complex, has been reported (9). The chemical purity was >96% with the specific activity of 1 Ci/μmol (37 GBq//μmol) at the EOS. The overall radiochemical yield was 23% at the EOS. The total synthesis time was 90 min. Nucleophilic methods using [^18^F]fluoride ion have the potential to provide a higher yield and a higher specific activity.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDOPA%5BAll%20Fields%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

The enzyme kinetic parameters for AAAD of DOPA and FDOPA were determined in vitro (10). The K_m_ and k_cat_ values for DOPA were 0.091 mM and 9.1 s^-1^, respectively. The K_m_ and k_cat_ values for FDOPA were 0.7 mM and 8.2 s^-1^, respectively. The presence of fluorine at ring position 6 decreased binding to the active site of AAAD without significantly affecting the enzyme activity of AAAD.

Unlabeled FDOPA (50 μM) reduced [^3^H]L-DOPA (25 nM) uptake by 69% and 49% in rat striatal and cortical synaptosomes, respectively. L-DOPA showed a higher inhibition than FDOPA (11). In another study, 3-OMFD, L-DOPA and unlabeled FDOPA inhibited the uptake of [^3^H]trytophan (0.1 μM) into cells transfected with human L-type amino acid transporter with IC_50_ of 84, 46, and 878 μM, respectively (12).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDOPA%5BAll%20Fields%5D%20AND%20rodentia)]

Ex vivo iodistribution studies showed a high uptake of radioactivity in the kidneys (5.6% ID/organ), pancreas (0.9% ID/organ) and liver (0.7% ID/organ) of mice at 1 h post injection of FDOPA (13).

Total extracellular [^18^F] radioactivity in rat striatum was observed to peak at 30 min after injection of FDOPA and declined with clearance half-life of 2 h (14). In the extracellular space, the dominant FDOPA metabolite at early times was FDOPAC, followed by FHVA at 50 min. F-sulfoconjugates appeared at 70 min, and finally 3-OMFD appeared later. Analysis of the striatal tissue confirmed the intraneuronal localization of FDA, most likely stored in vesicles, slowing its cerebral clearance.

In rat brain, carbidopa pretreatment increased striatal FDA (700%) and 3-OMFD (230%) at 30 min postinjection of FDOPA and cerebellum FDA (370%) and 3-OMFD (300%) (15). FDOPA plasma levels were increased by 20% and 3-OMFD plasma levels by 220%. FDOPAC and FDA were not detected. FHVA levels (>5%) were not changed by carbidopa pretreatment. Carbidopa restricted peripheral FDOPA metabolism to 3-OMFD formation and increased FDOPA bioavailability to the brain, resulting in greater FDA accumulation in the striatum.

The uptake of FDOPA was studied in a rat model of PD (16). The brains of these rats were unilaterally lesioned with an intranigral injection of 6-hydroxydopamine. The uptake in the lesioned side was 16-31% lower than the sham controls and intact side of the striatum and substantia nigra. The uptake data correlated with the behavioral tests and the number of nigral dopaminergic neurons.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDOPA%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

In dogs, FDOPA uptake was greatest in the pituitary, followed by the liver, spleen and kidneys at 1 h post injection. The uptake in the brain cortex, striatum, thalamus and cerebellum was <50% of the liver uptake (17).

FDOPA metabolism of immature brain was studied in newborn piglets (18). The estimated values of FDOPA decarboxylation in the basal ganglia were similar to values calculated in adult animals and humans. However, a significant FDOPA decarboxylation was also found in the frontal cortex and the cerebellum. HPLC analysis of brain samples also revealed extensive and rapid metabolism of FDOPA in the frontal cortex, caudate/putamen, midbrain, and cerebellum. At 8 min after tracer injection, about 80% of FDOPA was already converted to FDA and its metabolites. Surprisingly, a rather high fraction (16-21%) of [^18^F]fluoro-3-methoxytyramine was found, indicating a low storage capacity of vesicular dopamine at this perinatal stage. In a later study, it was found that the metabolism of FDOPA in young pigs was significantly faster than in newborns (19).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fdopa%20AND%20primate%20NOT%20human)]

FDOPA PET studies in non-human primates have provided useful assessment of the dopaminergic function in the brain. The major metabolite detected in the periphery was 3-OMFD (15). Carbidopa pretreatment increased FDOPA bioavailability to the brain and increased FDOPA metabolism to FDA and 3-OMFD. In the striatum, FDA and 3-OMFD were the major FDOPA metabolites with lower levels of FDOPAC and FHVA. In contrast, the cerebellum and cortex had mainly FDOPA and 3-OMFD accumulation (20-22).

Carbidopa pretreatment of monkeys showed inhibition of peripheral decarboxylation of FDOPA and higher uptake in the striatum and cortex than the control monkeys (15). There was no change in the FDOPA influx constant. Therefore, the higher uptake was because of higher FDOPA bioavailability for transport into the brain.

FDOPA metabolites from putamen of normal and 1-methyl-4-phenyl-1,2,3,6-tetrahydropyridine (MPTP)-treated monkeys were measured to correlate FDOPA metabolism with those of the endogenous dopamine system (23). There were less than 2% of control FDOPA and dopamine levels in the MPTP-treated putamen, which had 80% 3-OMFD as the major metabolite. FDA metabolism was increased for the lesioned putamen as measured by FHVA/FDA ratios (6:1 vs. 0.38:1). At 60 min post FDOPA injection, similar plasma activity for FDOPA and its metabolites were found for both control and lesioned monkeys. The results suggested that PET studies with FDOPA in PD patients could provide kinetic evaluation of striatal biochemistry and evidence of in vivo dopamine turnover changes.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fdopa%20AND%20human)]

Human dosimetry was estimated based on murine and human biodistribution data (13, 17). The bladder wall receives the highest dose (0.215 mGy/MBq or 0.797 rad/mCi). Other organs receiving high doses are the kidneys (0.089 mGy/MBq or 0.329 rad/mCi) and pancreas (0.030 mGy/MBq or 0.110 rad/mCi). The brain, liver and lungs receive <0.008 mGy/MBq (0.029 rad/mCi). Effective dose equivalent of 0.026 mSv/MBq (96 mrem/mCi) was estimated in the intravenous administration of FDOPA.

The first FDOPA PET study of human brain was reported in 1983 (24), showing the localization of radioactivity in the striatum. Only about 1% of FDOPA entered the brain. Striatal-to-occipital ratio, FDOPA influx constant, and AAAD activity constant are commonly used as analytical parameters in FDOPA PET studies. In patients with established bilateral PD, FDOPA PET showed bilateral influx constant reductions in the caudate, putamen, striatal nigra, and midbrain tegmentum. The decline in FDOPA uptake was more rapid in PD than normal subjects (25). In PD patients, AAAD activity was reduced in striatum, putamen, and caudate and no change in frontal and occipital cortices (26).

In carbidopa-pretreated subjects, peripheral FDOPA was rapidly metabolized by COMT to 3-OMFD. There were significant increases in FDOPA plasma levels for 30 min, but FHVA level decreased. Inhibition of COMT by entacapone in mild to moderate PD patients prolonged the circulation time of FDOPA in the plasma (27). but did not change rate constants for striatal FDOPA influx or decarboxylation. In advanced PD patients pretreated with entacapone, the FDOPA influx constant decreased significantly in the caudate and putamen, and no change in healthy controls. This may be because of the advanced disease, decreased storage capacity, or both (28).

FDOPA PET permits objective monitoring of PD progression and neuroprotection therapies [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fdopa%20AND%20Parkinson's%20disease)]. It allows diagnosis of PD in early disease stages. In recent studies, FDOPA has also demonstrated its usefulness as in the imaging of brain tumors (29) and neuroendocrine metastatic lesions in bone (30).

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Barrio J.R., Huang S.C., Phelps M.E. (1997). Biological imaging and the molecular basis of dopaminergic diseases. Biochem Pharmacol.
4 Heiss W.D., Hilker R. (2004). The sensitivity of 18-fluorodopa positron emission tomography and magnetic resonance imaging in Parkinson's disease. Eur J Neurol.
5 Thobois S., Guillouet S., Broussolle E. (2001). Contributions of PET and SPECT to the understanding of the pathophysiology of Parkinson's disease. Neurophysiol Clin.
6 Luxen A., Guillaume M., Melega W.P., Pike V.W., Solin O., Wagner R. (1992). Production of 6-[18F]fluoro-L-dopa and its metabolism in vivo--a critical review. Int J Rad Appl Instrum B.
7 Adam M.J., Ruth T.J., Grierson J.R., Abeysekera B., Pate B.D. (1986). Routine synthesis of L-[18F]6-fluorodopa with fluorine-18 acetyl hypofluorite. J Nucl Med.
8 Chang C.W., Wang H.E., Lin H.M., Chtsai C.S., Chen J.B., Liu R.S. (2000). Robotic synthesis of 6-[18F]fluoro-L-dopa. Nucl Med Commun.
9 Lemaire C., Damhaut P., Plenevaux A., Comar D. (1994). Enantioselective synthesis of 6-[fluorine-18]-fluoro-L-dopa from no-carrier-added fluorine-18-fluoride. J Nucl Med.
10 Borri Voltattorni C., Bertoldi M., Bianconi S., Deng W.P., Wong K., Kim I., Herbert B., Kirk K.L. (2002). Behavior of fluorinated analogs of L-(3,4-dihydroxyphenyl)alanine and L-threo-(3,4-dihydroxyphenyl)serine as substrates for Dopa decarboxylase. Biochem Biophys Res Commun.
11 Yee R.E., Cheng D.W., Huang S.C., Namavari M., Satyamurthy N., Barrio J.R. (2001). Blood-brain barrier and neuronal membrane transport of 6-[18F]fluoro-L-DOPA. Biochem Pharmacol.
12 Brust P., Vorwieger G., Walter B., Fuchtner F., Stark H., Kuwabara H., Herzau M., Opfermann T., Steinbach J., Ganapathy V., Bauer R. (2004). The influx of neutral amino acids into the porcine brain during development: a positron emission tomography study. Brain Res Dev Brain Res.
13 Mejia A.A., Nakamura T., Itoh M., Hatazawa J., Ishiwata K., Ido T., Matsumoto M., Watabe H., Watanuki S., Seo S. (1991). Absorbed dose estimates in positron emission tomography studies based on the administration of 18F-labeled radiopharmaceuticals. J Radiat Res (Tokyo).
14 DeJesus O.T., Haaparanta M., Solin O., Nickles R.J. (2000). 6-fluoroDOPA metabolism in rat striatum: time course of extracellular metabolites. Brain Res.
15 Melega W.P., Hoffman J.M., Luxen A., Nissenson C.H., Phelps M.E., Barrio J.R. (1990). The effects of carbidopa on the metabolism of 6-[18F]fluoro-L-dopa in rats, monkeys and humans. Life Sci.
16 Forsback S., Niemi R., Marjamaki P., Eskola O., Bergman J., Gronroos T., Haaparanta M., Haapalinna A., Rinne J., Solin O. (2004). Uptake of 6-[18F]fluoro-L-dopa and [18F]CFT reflect nigral neuronal loss in a rat model of Parkinson's disease. Synapse.
17 Harvey J., Firnau G., Garnett E.S. (1985). Estimation of the radiation dose in man due to 6-[18F]fluoro-L-dopa. J Nucl Med.
18 Brust P., Bauer R., Walter B., Bergmann R., Fuchtner F., Vorwieger G., Steinbach J., Johannsen B., Zwiener U. (1998). Simultaneous measurement of [18F]FDOPA metabolism and cerebral blood flow in newborn piglets. Int J Dev Neurosci.
19 Brust P., Walter B., Hinz R., Fuchtner F., Muller M., Steinbach J., Bauer R. (2004). Developmental changes in the activities of aromatic amino acid decarboxylase and catechol-O-methyl transferase in the porcine brain: a positron emission tomography study. Neurosci Lett.
20 Chan G.L., Doudet D.J., Dobko T., Hewitt K.A., Schofield P., Pate B.D., Ruth T.J. (1995). Routes of administration and effect of carbidopa pretreatment on 6-[18F]fluoro-L-dopa/PET scans in non-human primates. Life Sci.
21 Endres C.J., DeJesus O.T., Uno H., Doudet D.J., Nickles J.R., Holden J.E. (2004). Time profile of cerebral [18F]6-fluoro-L-DOPA metabolites in nonhuman primate: implications for the kinetics of therapeutic L-DOPA. Front Biosci.
22 Melega W.P., Grafton S.T., Huang S.C., Satyamurthy N., Phelps M.E., Barrio J.R. (1991). L-6-[18F]fluoro-dopa metabolism in monkeys and humans: biochemical parameters for the formulation of tracer kinetic models with positron emission tomography. J Cereb Blood Flow Metab.
23 Melega W.P., Hoffman J.M., Schneider J.S., Phelps M.E., Barrio J.R. (1991). 6-[18F]fluoro-L-dopa metabolism in MPTP-treated monkeys: assessment of tracer methodologies for positron emission tomography. Brain Res.
24 Garnett E.S., Firnau G., Nahmias C. (1983). Dopamine visualized in the basal ganglia of living man. Nature.
25 Vingerhoets F.J., Snow B.J., Lee C.S., Schulzer M., Mak E., Calne D.B. (1994). Longitudinal fluorodopa positron emission tomographic studies of the evolution of idiopathic parkinsonism. Ann Neurol.
26 Kuwabara H., Cumming P., Yasuhara Y., Leger G.C., Guttman M., Diksic M., Evans A.C., Gjedde A. (1995). Regional striatal DOPA transport and decarboxylase activity in Parkinson's disease. J Nucl Med.
27 Ishikawa T., Dhawan V., Chaly T., Robeson W., Belakhlef A., Mandel F., Dahl R., Margouleff C., Eidelberg D. (1996). Fluorodopa positron emission tomography with an inhibitor of catechol-O-methyltransferase: effect of the plasma 3-O-methyldopa fraction on data analysis. J Cereb Blood Flow Metab.
28 Ruottinen H.M., Rinne J.O., Ruotsalainen U.H., Bergman J.R., Oikonen V.J., Haaparanta M.T., Solin O.H., Laihinen A.O., Rinne U.K. (1995). Striatal [18F]fluorodopa utilization after COMT inhibition with entacapone studied with PET in advanced Parkinson's disease. J Neural Transm Park Dis Dement Sect.
29 Becherer A., Karanikas G., Szabo M., Zettinig G., Asenbaum S., Marosi C., Henk C., Wunderbaldinger P., Czech T., Wadsak W., Kletter K. (2003). Brain tumour imaging with PET: a comparison between [18F]fluorodopa and [11C]methionine. Eur J Nucl Med Mol Imaging.
30 Becherer A., Szabo M., Karanikas G., Wunderbaldinger P., Angelberger P., Raderer M., Kurtaran A., Dudczak R., Kletter K. (2004). Imaging of advanced neuroendocrine tumors with (18)F-FDOPA PET. J Nucl Med.